# Trastuzumab conjugated to tetramethyl-6-carboxyrhodamine-QSY^®^7

Chemical name: | Trastuzumab conjugated to tetramethyl-6-carboxyrhodamine-QSY^®^7
Abbreviated name: | Traz-TM-Q7
Synonym:
Agent Category: | Receptor ligand
Target: | Human epidermal growth factor 2 (HER2)
Target Category: | Receptor
Method of detection: | Optical imaging: fluorescence
Source of signal / contrast: | Tetramethyl-6-carboxyrhodamine
Activation: | Yes
Studies: | - In vitro; - Rodents | Click here for information regarding human EGFR. (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=databasead&logdbfrom=protein)

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=fluorophore+quencher+optical+probes)]

Early detection of cancer helps in the development of a proper treatment and monitoring regimen that may result in a suitable prognosis for the patient (1-3). Although invasive methods are often used for the detection of cancer, these procedures have limitations because they may detect the neoplasm only in a specific location and cannot determine whether the cancer has metastasized to other parts of the body. In addition, the various imaging techniques and modalities available for the non-invasive detection of cancer have low sensitivity and resolution, which are insufficient to detect and quantify microscopic tumors or a small cluster of cancerous cells (4), and some of the contrast agents used for imaging purposes are known to have toxic side effects (5). An attractive alternative to radionuclides or contrast agents is the use of fluorescent optical imaging agents that was used to visualize and manage or treat clinical pathologies, including that of cancer in small animals (6-9). However, fluorescent dyes used for imaging can be toxic or nonspecific, and the signal generated by these agents may be masked by autofluorescence, leading to a low signal/background ratio (10). Investigators have proposed the use of targeted fluorescent probes as a solution to improve the signal/background ratio with optical imaging agents, and it was shown that a fluorescent dye conjugated to avidin or a monoclonal antibody (MAb) such as trastuzumab (Traz) can be used to detect submillimeter disseminated tumors under in vitro and in vivo conditions (11-13). It is important to mention here that currently fluorescent dyes can be used only to visualize only surface tumors or after exposure of the tumor if it is present in a body cavity (e. g. peritoneum).

The human epidermal growth factor receptor (HER; it has several isoforms: HER1, HER2, HER3, and HER4) plays an important role in the development of various neoplasms (14-16). Once a ligand is bound to HER, a tyrosine kinase signaling pathway is activated, which initiates cell growth and division that can lead to the development and progression of cancer. Soon after the signaling pathway is activated, the receptor-ligand complex is internalized by the cell for inactivation by enzymatic digestion in the lysosome (17). Because of their role in the cancer process, several commercially available humanized MAbs directed toward HER, including Traz, are approved by the United States Food and Drug Administration to treat cancers. Traz specifically targets the HER2 receptor and is used either as a primary agent or as an adjuvant for the treatment of breast cancer in the clinical setting (18). It is also under investigation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=trastuzumab) for the treatment of other neoplasms.

Ogawa et al. proposed the use of fluorophores that could be activated only after binding to the target to further improve the target/background ratios obtained with the optical imaging agents (13). These investigators developed a targeted and activatable fluorophore-quencher (FQ) probe that could be used for the optical imaging of tumors. The chemical structure of the FQ probe was designed so that, in the native state, the signal from the fluorophore is quenched by a quencher molecule. However, a fluorescence signal would be obtained from the fluorophore only after the FQ probe was bound to, internalized, and activated (by degradation of the targeting molecule, in this case the MAb) in the target cells. The mechanism of quenching and generating fluorescence from the FQ probe is discussed in detail elsewhere (19). Ogawa et al. investigated the use of tetramethyl-6-carboxyrhodamine (TAMRA, fluorophore)-QSY^®^7 (quencher) pair conjugated to Traz (Traz-TM-Q7) for the detection of cancer cells under in vitro conditions and in mice bearing NIH3T3 cell tumors. These cells had previously been transfected with the HER2 gene (3T3/HER2+). Normal NIH3T3 cells (Balb/3T3/Her2-) cells were used as controls for this study (13).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TAMRA+QSY7+avidin+synthesis)]

The synthesis of Traz-TM-Q7 was described by Ogawa et al. (13). Briefly, Traz was incubated with QSY^®^7-hydroxysuccinimide (NHS) ester (dissolved in dimethylsulfoxide) in 0.1 M sodium phosphate buffer (Na_2_HPO_4_) (pH 8.5) for 30 min at room temperature. The Traz- QSY^®^7 conjugate was purified on a Sephadex G50 column, concentrated, and added to a solution of TAMRA-NHS. The mixture was incubated as described above, and the final product, Traz-TM-Q7, was purified on a Sephadex G50 column. Purified Traz-TM-Q7 was stored at 4°C until needed. The stability of Traz-TM-Q7 under these storage conditions was not reported. Approximately one and three molecules of TAMRA and QSY^®^7, respectively, were reported to be conjugated to each molecule of Traz, as determined with a spectroscopic system after denaturation with 5% sodium dodecylsulfate (SDS). A TAMRA conjugate of Traz (Traz-TM) was also generated by incubating Traz with TAMRA-NHS for 30 min at room temperature. Traz-TM was purified as described above, and the purified product was stored at 4°C. The stability of Traz-TM was not reported.

To generate a control for use in some studies, a TAMRA-QSY®7 conjugate of daclizumab (a MAb that is specific for HER1) was generated (Dac-TM-Q7) using a protocol similar to that described for the Traz conjugate (13). For use as a control, the TAMRA conjugate of Dac lacking QSY-7 (Dac-TM) was also prepared as described above. The purification and stability of Dac-TM-Q7 and Dac-TM were not reported. In addition, the number of TAMRA-QSY-7 or TMARA conjugated to each daclizumab molecule was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=trastuzumab+tamra+qsy7+in+vitro)]

The quenching ability of the MAb conjugates was determined by denaturing them with 5% SDS containing 2-mercaptoethanol (2-ME) in phosphate-buffered saline (PBS) for 2 min at 95°C (13). For comparison, the two MAb-TM conjugates were incubated in PBS under the same conditions. Measurement of the fluorescence signal from each denatured sample showed that only the dissociated MAb conjugate samples had an increase in fluorescent signal over background. The Traz-TM-Q7 and the Traz-Tm conjugates exhibited 13- and 3-fold increases in fluorescence, respectively. For the Dac-TM-Q7 and Dac-TM conjugates, 9- and 4-fold increases were reported, respectively. The increase in fluorescence of the Traz-TM and Dac-TM conjugates was attributed to an intrinsic characteristic of rhodamine containing fluorophores that are activated after internalization by the cells (the rhodamine effect) (20).

To demonstrate intracellular activation of Traz-TM-Q7, Traz-TM, Dac-TM-Q7, and the Dac-TM conjugates, 3T3/HER2+ cells were exposed to the respective conjugates at 37°C for either 1 or 8 h to allow internalization and activation of the fluorophore in the lysosomes (13). An examination of the exposed cells under a fluorescence microscope after 1 h exposure to Traz-TM-Q7 or Traz-TM showed that the fluorescence was visible only on the cell surface. At 8 h after exposure, the fluorescent dots were visible in the lysosomes of the cells, indicating that the Traz-TM-Q7 and Traz-TM conjugates had been internalized by the cells. Fluorescence from cells exposed to Traz-TM-Q7 was reported to be higher than that from cells treated with the Traz-TM conjugate. No fluorescent signal was obtained from cells treated with either Dac-TM-Q7 or Dac-TM because these conjugates did not target HER2 and did not bind to or were not internalized by the 3T3/HER2+ cells. Pre-exposure of the 3T3/HER2+ cells to unlabeled Traz (at a concentration equal to the Traz fluorescent conjugates) was reported to reduce the fluorescence signal obtained from Traz-TM-Q7 treatment of the cells. This indicated that the conjugated MAb had a binding specificity similar to unlabeled Traz.

In another study to investigate the intracellular localization of Traz-TM-Q7, 3T3/HER2+ tumors were removed from the lungs of mice (see below for details) and treated with a commercially available fluorescent lysosomal marker 30 min before exposure to the MAb conjugate. The tumor cells were then observed under a fluorescent microscope. The fluorescent signals from the lysosomal marker and Traz-TM-Q7 were reported to have a similar location in the cells, indicating that the MAb conjugate was internalized by the cells and degraded in the lysosomes.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=trastuzumab+tamra+qsy7+rodentia)]

The uptake of Traz-TM-Q7, Traz-Tm, Dac-TM-Q7, and Dac-TM was investigated in mice bearing 3T3/HER2+ tumors in the lungs (13). Imaging was performed on the animals (5 mice/MAb conjugate) 1 d after intravenous injection of the respective MAb conjugates through the tail vein. A low background was reported with Traz-TM-Q7, whereas nonspecific fluorescence was obtained with Traz-TM. The tumor/normal lung tissue fluorescence ratios were reported to be significantly higher (P < 0.01) for Traz-TM-Q7 (22.4 ± 4.3) than for Traz-TM (5.7 ± 1.8). Pretreatment of the tumor-bearing mice with unlabeled Traz (~13 μmol/animal) reduced the accumulation of both MAb conjugates in the tumors and the surrounding lung tissues (tumor/normal lung tissue ratios were not reported). With Dac-TM-Q7, a very low fluorescent signal was observed in the lungs, but Dac-TM generated a generalized signal in the organs.

To determine the sensitivity and specificity of Traz-TM-Q7, mice with the NIH3T3/HER2+ and NIH3T3/HER2-/ZsGreen cell tumors (these cells constitutively express the green fluorescence protein) were injected with the MAb conjugate and imaged 1 d after the treatment; the number of animals injected with each conjugate was not reported (13). No overlap of the fluorescent signal from TAMRA and ZsGreen was observed in tumors of these animals because the NIH3T3/HER2-/ZsGreen cell tumors did not express any HER2.

On the basis of the information obtained from the various studies performed with Traz-TM-Q7, the investigators concluded that this activatable FQ probe could probably be used to manage cancer with a “see and treat” strategy (13).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=trastuzumab+tamra+qsy7+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=trastuzumab+tamra+qsy7+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=trastuzumab+tamra+qsy7+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Some of the work presented in this chapter was supported by the Intramural Research Program of the National Institutes of Health, National Cancer Institute, and the Center for Cancer Research.

## References

1 Brepoels L., Stroobants S. (2008). PET scanning and prognosis in Hodgkin's lymphoma. Curr Opin Oncol.
2 Dobbe E., Gurney K., Kiekow S., Lafferty J.S., Kolesar J.M. (2008). Gene-expression assays: new tools to individualize treatment of early-stage breast cancer. Am J Health Syst Pharm.
3 Kolesar J.M. (2008). Assessing therapeutically developed assays. Manag Care.
4 Frangioni J.V. (2008). New technologies for human cancer imaging. J Clin Oncol.
5 ten Dam M.A., Wetzels J.F. (2008). Toxicity of contrast media: an update. Neth J Med.
6 Xiao W., Yao N., Peng L., Liu R., Lam K.S. (2009). Near-infrared optical imaging in glioblastoma xenograft with ligand-targeting alpha 3 integrin. Eur J Nucl Med Mol Imaging.
7 Sampath L., Wang W., Sevick-Muraca E.M. (2008). Near infrared fluorescent optical imaging for nodal staging. J Biomed Opt.
8 van de Ven S.M., Elias S.G., van den Bosch M.A., Luijten P., Mali W.P. (2008). Optical imaging of the breast. Cancer Imaging.
9 Thekkek N., Richards-Kortum R. (2008). Optical imaging for cervical cancer detection: solutions for a continuing global problem. Nat Rev Cancer.
10 Aalders M.C. (1999). N. vd Vange, F.A. Stewart, M.G. Klein, M.J. vd Vijver, and H.J. Sterenborg, White-light toxicity, resulting from systemically administered 5-aminolevulinic acid, under normal operating conditions. J Photochem Photobiol B.
11 Hama Y., Urano Y., Koyama Y., Kamiya M., Bernardo M., Paik R.S., Krishna M.C., Choyke P.L., Kobayashi H. (2006). In vivo spectral fluorescence imaging of submillimeter peritoneal cancer implants using a lectin-targeted optical agent. Neoplasia.
12 Hama Y., Urano Y., Koyama Y., Choyke P.L., Kobayashi H. (2006). Targeted optical imaging of cancer cells using lectin-binding BODIPY conjugated avidin. Biochem Biophys Res Commun.
13 Ogawa, M., N. Kosaka, M.R. Longmire, Y. Urano, P.L. Choyke, and H. Kobayashi, Fluorophore-quencher based activatable targeted optical probes for detecting in vivo cancer metastases. Mol Pharm, 2009
14 Weber J., McCormack P.L. (2008). Panitumumab: in metastatic colorectal cancer with wild-type KRAS. BioDrugs.
15 Mehra R., Cohen R.B., Burtness B.A. (2008). The role of cetuximab for the treatment of squamous cell carcinoma of the head and neck. Clin Adv Hematol Oncol.
16 Hall P.S., Cameron D.A. (2009). Current perspective - trastuzumab. Eur J Cancer.
17 Woodman P. (2009). ESCRT proteins, endosome organization and mitogenic receptor down-regulation. Biochem Soc Trans.
18 Simonds H.M., Miles D. (2007). Adjuvant treatment of breast cancer: impact of monoclonal antibody therapy directed against the HER2 receptor. Expert Opin Biol Ther.
19 Lee S., Park K., Kim K., Choi K., Kwon I.C. (2008). Activatable imaging probes with amplified fluorescent signals. Chem Commun (Camb).
20 Longmire M.R., Ogawa M., Hama Y., Kosaka N., Regino C.A., Choyke P.L., Kobayashi H. (2008). Determination of optimal rhodamine fluorophore for in vivo optical imaging. Bioconjug Chem.